# Carbobenzoxy-capped Phe-Lys(BODIPY TMR-X-acyloxymethyl ketone(QSY7)

Chemical name: | Carbobenzoxy-capped Phe-Lys(BODIPY TMR-X)-acyloxymethyl ketone(QSY7)
Abbreviated name: | GB117
Synonym: | Quenched activity-based probe (qABP)
Agent Category: | Compounds
Target: | Cysteine cathepsin
Target Category: | Enzyme
Method of detection: | Optical imaging
Source of signal / contrast: | BODIPY TMR-X
Activation: | Yes
Studies: | - In vitro | Click on the PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=cathepsin) for additional information of the relevant substances.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cysteine+cathepsins)]

The human cysteine cathepsins have 11 members (cathepsins B, C, H, F, K, L, O, S, V, W, and X/Z) and share a conserved active site that is formed by cysteine, histidine, and asparagine residues (1-5). Cathepsins B, L, H, F, O, X/Z, and C are expressed ubiquitously, whereas the expression of cathepsins S, K, W, and V are relatively organ-limited. Cysteine cathepsins interact with other proteases (aspartic, metallo, serine, and threonine) in a cascade-like manner, involving various physiological processes, including protein degradation, precursor protein activation, MHC-II–mediated antigen presentation, bone remodeling, keratinocytes differentiation, hair follicle cycle, reproduction, and apoptosis (6, 7). Increased expression and activity, and relocalization to the plasma membrane of cysteine cathepsins are associated with the pathogenesis of a number of human diseases such as cancer, atherosclerosis, and neurodegenerative diseases, and changes related to cysteine cathepsins have been shown to be of diagnostic and prognostic value for the diseases (2, 8-11).

Significant efforts have been made in developing optical molecular probes of protease activity (4, 7, 12, 13). These probes are either substrate-based or activity-based, providing a readout of the enzyme activity rather than simple protein abundance. Substrate-based probes (SBPs) are designed using fluorescent peptide sequences tethered to a large polymer or dendramer backbone, and these SBPs are internally quenched by the high density of fluorophores loaded onto the backbone structure. Similar to conventional enzymatic tests, SBPs appear to be less reliable because of overlapping substrate specificities, enzymatic activity instability, and interactions with endogenous inhibitors. Activity-based probes (ABPs) label target proteases through the formation of a covalent bond with the active site cysteine. The selectivity of an ABP is controlled by both its peptide selectivity sequence and reactive functional group. The fluorescent reporter allows probe-labeled cathepsins to be directly visualized. Because ABPs tend to be small molecules, the in vivo half-lives of ABPs are relatively short, which results in the production of high-contrast images. A drawback of using a covalent probe is the lack of signal amplification because the target proteases are inactivated upon binding the probe. However, sufficient levels of the active proteases have been found to exist in tumor tissues, which allows the generation of reasonable contrast images using noninvasive methods (4, 7, 12).

Blum et al. synthesized a group of near-infrared fluorescent activity-based probes (NIRF-ABPs) for noninvasive optical imaging of cysteine protease activity (4, 7, 12, 14). These probes can be subgrouped into quenched ABPs (qABPs) (e.g., GB117, GB119, GB135, and GB137) and nonquenched ABPs (e.g., GB111, GB123, and GB138). In short, the probes consist of a reactive group of peptide acyloxymethyl ketone (AOMK) that targets diverse members of cysteine cathepsins. The ketone in AOMK reacts with the cysteine in the enzyme active site and produces a stable thiomethyl ketone adduct. The covalent binding involves the loss of the acyloxy group of AOMK. Thus, a probe carrying a fluorescent reporter group on its peptide scaffold and a highly efficient quenching molecule attached to the acyloxy-losing group should result in a quenched probe that only becomes fluorescent upon covalent binding with an enzyme. In addition, a spacer is designed to reduce the steric congestion between the reporter and the fluorescence quencher. Blum et al. have shown that the NIRF-ABPs are nontoxic to cells, reasonably water soluble, potentially valuable as imaging agents for disease diagnosis, and powerful tools for in vivo preclinical and clinical testing of small-molecule therapeutic agents. Although NIRF-ABPs present different features regarding stability, specificity, and kinetics, the quenched probes can be used to image specific protease activity at considerably earlier time points than can be used for substrate-based methods or nonquenched ABPs. However, high levels of signal in large organs with high cathepsin activity such as liver, kidney, and spleen make activity-based imaging of specific locations within the central body cavity difficult. In this chapter, the synthesis and analytic results of quenched GB117 were introduced, which were compared with that of GB111. The quenched GB117 and its corresponding nonquenched control GB111 are the first generation of this group of NIRF-ABPs.

### Related Resource Links:

1) Cysteine cathepsin imaging-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html):

- Substrate-based probes: Cy5.5-PL-MPEG (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=PL-MPEG-Cy55), Cy5.5-GHPGGPQK(Fitc)C-PL-MPEG (Cy5.5-CatK-PGC) (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=CatK-PL-MPEG-Cy55)
- Activity-based probes: GB137 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=GB137)

2) Gene and protein information of human cathepsins (http://www.ncbi.nlm.nih.gov/protein/?term=cathepsin+and+human)

3) Cathepsin-related resource in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=cathepsin)

4) Cathepsin-related substances in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=cathepsin)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

Blum et al. described a four-step synthesis of the probes GB117 and GB111 (12). The investigators first synthesized the fully protected carbobenzoxy-capped Phe-Lys dipeptide using standard solid-phase peptide synthesis (85% purity and 99% yield relative to resin loading). The investigators then converted the dipeptide to bromo-methyl ketone (BMK, 91% yield). A subsequent conversion of the BMK via N-trityl–protected glycine yielded AOMK (25% yield). As the final step, GB117 was generated by coupling the QSY7-quenched group after removal of the trityl group and by coupling the BODIPY-TMR-X fluorophore (excitation/emission is 544/570 nm) after removal of the t-butoxy carbonyl–protecting group on the side chain of lysine (72% yield). In contrast to GB117, the QSY7-quenched group was not coupled for the control GB111 (58% yield). The molecular weights were 1,632.7 and 1,089.6 for GB117 and GB111, respectively (12).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

Blum et al. evaluated the quenching of fluorescent signals and the effect of fluorophore attachment on the probe potency toward cathepsins (12). Attachment of the fluorophore to the P1 lysine side chain resulted in >70-fold increased fluorescent quenching for GB117 compared with the nonquenched GB111. Fluorophore attachment to the more distal positions (i.e., P2, P3, or the amino terminus) also led to sufficient quenching for imaging applications (data not shown). Because the majority of the critical substrate interactions take place in the P2 position of the papain-family proteases, Blum et al. selected the P1 position for fluorophore attachment in developing probes. After attachment, GB111 exhibited a 100-fold loss of potency toward cathepsin L and a 30-fold loss of potency for cathepsin B when compared with its free amine intermediate (NH_2_-GB111). Interestingly, replacement of the 2,6-methyl benzoyl group with the QSY7 quencher resulted in a larger decrease in the potency of GB117 toward cathepsin B than toward cathepsin L. The investigators explained this phenomenon by postulating that the QSY7 group potentially produced van der Waals clashes with the occluding loop of cathepsin B. The apparent rate constant (K_app_) of GB111 was 2,580 ± 800 and 1,256 ± 308 for cathepsins L and B, respectively. The K_app_ of GB117 was 7,000 ± 1,200 and 275 ± 66 for cathepsins L and B, respectively. These results suggest that GB117 is more specific to cathepsin L than to cathepsin B.

Blum et al. tested the labeling of cathepsins B and L with these probes with the use of purified recombinant cathepsins in intact cells (12). Both GB111 and GB117 labeled the enzymes through a stable covalent linkage. This labeling can be specifically countered with pretreatment of the enzymes with a broad-spectrum, papain-family cysteine protease inhibitor JPM-OEt (15). However, the investigators noticed that both GB111 and GB117 also labeled other purified cathepsins (cathepsins X and S; data not shown), suggesting that these probes may label multiple targets. In intact NIH-3T3 cells, both probes have been shown to label endogenous enzyme targets after incubation of the cells with the probes. Under microscopy, incubation of the NIH-3T3 cells with GB111 resulted in an intense, nonspecific labeling of the entire cell when imaged without washing, suggesting that GB111 does not accumulate in any particular location but distributes throughout the cell. On the contrary, a unique labeling pattern for GB117 was observed, which overlapped with the signal from the acidotropic lysosomal marker Lysotracker. The cell labeling can be blocked with pretreatment of the cells with inhibitor JPM-OEt for 1 h. With extensive washing after incubation of the cells with GB111, a labeling pattern similar to that seen with GB117 was observed. GB117 had a slower rate of modification than did GB111, suggesting that extended labeling times would be required to obtain optimal signal. SDS-PAGE analysis of the extracts of wild-type, cathepsin B–deficient, and cathepsin L–deficient fibroblast cells have further confirmed that GB117 is more specific to cathepsin L than to cathepsin B. These results indicate that both probes freely penetrate cells and label a series of protease targets with a high selectivity to cathepsins L and B. GB117 is fluorescently activated upon binding to protease targets and provides sufficient signal over noise to allow direct real-time analysis of protease activity in live cells.

To further confirm the feasibility of GB117 in imaging protease activity, Blum et al. evaluated the probes using a three-dimensional MCF-10A cell model that more accurately mimics human cancer (12). The fibrocystic breast cell line MCF-10A forms highly organized three-dimensional spheroids with glandular architecture when grown on reconstituted basement membranes (or matrix), and this line is considered to be an excellent cellular model for various forms of tumor growth. After 3 days of cell growth on the matrix containing GB111, direct imaging without washing produced a bright, nonspecific, intracellular fluorescent staining. The free probe in the matrix did not show any significant fluorescence, which suggested a quenching effect by matrix proteins. When the spheroids were washed and fixed, a specific staining pattern was observed, which was partially overlapped with immunofluorescent staining of the same fixed cells with an anti-cathepsin B antibody. Cells incubated on the matrix containing GB117 demonstrated a distinct punctate staining of the lysosomal compartments, and this staining was completely blocked by addition of the JPM-OEt, which suggested a specific staining of the active proteases. The population of active cathepsin B labeled by the probes was found predominantly at the apical pole of the cells in the acini, although the total distribution of cathepsin B protein was both apical and basal. These results further support the specific nature of the ABPs and also highlight the difference in imaging active protease populations rather than total protein levels with antibodies that recognize both precursor and active forms of proteases.

Blum et al. concluded that qABPs can be used to dynamically image protease activity in real time. It should be possible to apply this methodology to a range of diverse cysteine proteases. The use of this quenched-probe strategy can be adapted easily to incorporate near-infrared tags that may facilitate noninvasive, whole-body imaging applications. One of the main limitations to this strategy is the lack of signal amplification, which potentially reduces the probe utility for whole-body imaging (4, 7, 12, 14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Colbert J.D., Matthews S.P., Miller G., Watts C. (2009). Diverse regulatory roles for lysosomal proteases in the immune response. Eur J Immunol.
2 Affara N.I., Andreu P., Coussens L.M. (2009). Delineating protease functions during cancer development. Methods Mol Biol.
3 Cox J.L. (2009). Cystatins and cancer. Front Biosci.
4 Blum G., von Degenfeld G., Merchant M.J., Blau H.M., Bogyo M. (2007). Noninvasive optical imaging of cysteine protease activity using fluorescently quenched activity-based probes. Nat Chem Biol.
5 Hang H.C., Loureiro J., Spooner E., van der Velden A.W., Kim Y.M., Pollington A.M., Maehr R., Starnbach M.N., Ploegh H.L. (2006). Mechanism-based probe for the analysis of cathepsin cysteine proteases in living cells. ACS Chem Biol.
6 Palermo C., Joyce J.A. (2008). Cysteine cathepsin proteases as pharmacological targets in cancer. Trends Pharmacol Sci.
7 Blum G. (2008). Use of fluorescent imaging to investigate pathological protease activity. Curr Opin Drug Discov Devel.
8 Cavallo-Medved D., Rudy D., Blum G., Bogyo M., Caglic D., Sloane B.F. (2009). Live-cell imaging demonstrates extracellular matrix degradation in association with active cathepsin B in caveolae of endothelial cells during tube formation. Exp Cell Res.
9 Gounaris E., Tung C.H., Restaino C., Maehr R., Kohler R., Joyce J.A., Ploegh H.L., Barrett T.A., Weissleder R., Khazaie K. (2008). Live imaging of cysteine-cathepsin activity reveals dynamics of focal inflammation, angiogenesis, and polyp growth. PLoS One.
10 Lutgens S.P., Cleutjens K.B., Daemen M.J., Heeneman S. (2007). Cathepsin cysteine proteases in cardiovascular disease. FASEB J.
11 Joyce J.A., Baruch A., Chehade K., Meyer-Morse N., Giraudo E., Tsai F.Y., Greenbaum D.C., Hager J.H., Bogyo M., Hanahan D. (2004). Cathepsin cysteine proteases are effectors of invasive growth and angiogenesis during multistage tumorigenesis. Cancer Cell.
12 Blum G., Mullins S.R., Keren K., Fonovic M., Jedeszko C., Rice M.J., Sloane B.F., Bogyo M. (2005). Dynamic imaging of protease activity with fluorescently quenched activity-based probes. Nat Chem Biol.
13 Yang Z., Fonovic M., Verhelst S.H., Blum G., Bogyo M. (2009). Evaluation of alpha,beta-unsaturated ketone-based probes for papain-family cysteine proteases. Bioorg Med Chem.
14 Blum G., Weimer R.M., Edgington L.E., Adams W., Bogyo M. (2009). Comparative assessment of substrates and activity based probes as tools for non-invasive optical imaging of cysteine protease activity. PLoS One.
15 Schurigt U., Sevenich L., Vannier C., Gajda M., Schwinde A., Werner F., Stahl A., von Elverfeldt D., Becker A.K., Bogyo M., Peters C., Reinheckel T. (2008). Trial of the cysteine cathepsin inhibitor JPM-OEt on early and advanced mammary cancer stages in the MMTV-PyMT-transgenic mouse model. Biol Chem.